# ^64^Cu-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-cyclo(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-cyclo(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | ^64^Cu-NODAGA-c(RGDyK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=23831237), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56237028) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about Integrin α_v_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20RGDfK)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (50% inhibition concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins (11). Various radiolabeled cyclic RGD peptides and peptidomimetics have been found to have high accumulation in tumors in mice (12, 13). From these developments, [^18^F]galacto-c(RGDfK) has been evaluated in a number of clinical studies for the imaging of α_v_β_3_ in cancer patients (14-18). Knetsch et al. (19) reported the development of ^68^Ga-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-cyclo(Arg-Gly-Asp-D-Phe-Lys) (^68^Ga-NODAGA-c(RGDfK)) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing melanoma tumors. 1-(1-Carboxy-3-carbo-tert-butoxypropyl)-4,7-(carbo-tert-butoxymethyl)-1,4,7-triazacyclononane (NODAGA(tBu)_3_) was used to prepare ^68^Ga-NODAGA-c(RGDfK). Dumont et al. (20) chelated NODAGA-c(RGDfK) with ^64^Cu to form ^64^Cu-NODAGA-c(RGDfK) for use with PET imaging of α_v_β_3_ receptors in nude mice bearing human glioblastoma tumors. However, renal and liver excretion of ^64^Cu-NODAGA-c(RGDfK) was slow. Oxboel et al. (21) prepared ^64^Cu-NODAGA-c(Arg-Gly-Asp-D-Tyr-Lys) (^64^Cu-NODAGA-c(RGDyK)) to increase renal excretion of the tracer since D-Tyr is more hydrophilic than D-Phe.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+synthesis)]

NODAGA-c(RGDyK) with NODAGA conjugation of the amino group of Lys (K) is commercially available. ^64^Cu-NODAGA-c(RGDyK) was prepared by reacting 2 nmol NODAGA-c(RGDyK) with 50–60 MBq (1.35–1.62 mCi) ^64^CuCl_2_ in ammonium acetate solution (pH 8.5) for 15 min at room temperature (21). ^64^Cu-NODAGA-c(RGDyK) was used without further purification and yielded a radiochemical purity of 93%–97% as determined with high-performance liquid chromatography. The specific activity was 25.3 MBq/nmol (0.68 mCi/nmol). ^64^Cu-NODAGA-c(RGDyK) remained >93% and 88% intact in the ammonium acetate buffer and mouse plasma after incubation for 24 h at room temperature, respectively. The hydrophilicity of ^64^Cu-NODAGA-c(RGDyK) was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+in+vitro)]

Human lung bronchus carcinoid H727 tumors from nude mice exhibited high gene expression of human and mouse α_v_ and VEGF-A as measured with quantitative real-time polymerase chain reaction (21). Expression of β_3_ was low for both species. No other in vitro studies (such as receptor binding, cellular accumulation) were performed with ^64^Cu-NODAGA-c(RGDyK).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+rodentia)]

Oxboel et al. (21) performed ex vivo biodistribution studies of 2 MBq (0.05mCi) ^64^Cu-NODAGA-c(RGDyK) in nude mice (n = 5/group) bearing α_v_β_3_-positive H272 tumors. The accumulation in tumors was 1.2 ± 0.2% injected dose/gram (ID/g), 0.7 ± 0.1% ID/g, and 0.6 ± 0.1% ID/g at 1, 2, and 18 h after intravenous injection, respectively. The organ with the highest accumulation at 1 h after injection was the kidney (2.2% ID/g), followed by the intestine (1.6% ID/g), liver (1.1% ID/g), and spleen (0.9% ID/g). The blood and muscle had radioactivity levels of <0.3% ID/g at 1 h. The washout from these normal tissues was rapid. The tumor/blood ratios were 12.7, 37.2, and 20.2 at 1, 2, and 18 h, respectively. The tumor/muscle ratios were 5.0, 7.3, and 7.1 at 1, 2, and 18 h after injection, respectively. There was significant correlation of tumor radioactivity at 2 h with mouse α_v_ integrin (R = 0.75, P < 0.05), mouse VEGF-A (R = 0.81, P < 0.05), and human α_v_ integrin (R = 0.86, P < 0.01)_._ No blocking studies were performed.

PET imaging was performed in a nude mouse bearing H272 tumors injected with 1.6 MBq (0.04 mCi) ^64^Cu-NODAGA-c(RGDyK) and imaged at 1, 2, and 18 h after injection (21). The tumors showed good contrast at 1 h after injection. The tumor radioactivity accumulation was 1.15%, 0.99%, and 0.76% ID/g at 1, 2, and 18 h after injection, respectively. The tumor/muscle ratios were 6.9 ± 0.8 at these time points. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA+RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
13 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
14 Beer A.J., Grosu A.L., Carlsen J., Kolk A., Sarbia M., Stangier I., Watzlowik P., Wester H.J., Haubner R., Schwaiger M. (2007). [18F]galacto-RGD positron emission tomography for imaging of alphavbeta3 expression on the neovasculature in patients with squamous cell carcinoma of the head and neck. Clin Cancer Res.
15 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.
16 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
17 Beer A.J., Lorenzen S., Metz S., Herrmann K., Watzlowik P., Wester H.J., Peschel C., Lordick F., Schwaiger M. (2008). Comparison of integrin alphaVbeta3 expression and glucose metabolism in primary and metastatic lesions in cancer patients: a PET study using 18F-galacto-RGD and 18F-FDG. J Nucl Med.
18 Beer A.J., Niemeyer M., Carlsen J., Sarbia M., Nahrig J., Watzlowik P., Wester H.J., Harbeck N., Schwaiger M. (2008). Patterns of alphavbeta3 expression in primary and metastatic human breast cancer as shown by 18F-Galacto-RGD PET. J Nucl Med.
19 Knetsch P.A., Petrik M., Griessinger C.M., Rangger C., Fani M., Kesenheimer C., von Guggenberg E., Pichler B.J., Virgolini I., Decristoforo C., Haubner R. (2011). [(68)Ga]NODAGA-RGD for imaging alpha(v)beta (3) integrin expression. Eur J Nucl Med Mol Imaging.
20 Dumont R.A., Deininger F., Haubner R., Maecke H.R., Weber W.A., Fani M. (2011). Novel (64)Cu- and (68)Ga-labeled RGD conjugates show improved PET imaging of alpha(nu)beta(3) integrin expression and facile radiosynthesis. J Nucl Med.
21 Oxboel J., Schjoeth-Eskesen C., El-Ali H.H., Madsen J., Kjaer A. (2012). (64)Cu-NODAGA-c(RGDyK) Is a Promising New Angiogenesis PET Tracer: Correlation between Tumor Uptake and Integrin alpha(V)beta(3) Expression in Human Neuroendocrine Tumor Xenografts. Int J Mol Imaging.